# Gly-Ala-Cys-Leu-Arg-Ser-Gly-Arg-Gly-Cys-Gly-(PEG)_3_-DOTA-^68^Ga

Chemical name: | Gly-Ala-Cys-Leu-Arg-Ser-Gly-Arg-Gly-Cys-Gly-(PEG)_3_-DOTA-^68^Ga
Abbreviated name: | ^68^Ga-DOTA-TCTP-1
Synonym:
Agent category: | Peptide
Target: | Gelatinase B (matrix metalloproteinase 9, MMP-9)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal/contrasat: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on MMP-9 (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=10443048) for protein information.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TCTP-1)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Several families of proteases are involved in atherogenesis, inflammation, myocardial infraction, angiogenesis, and tumor invasion and metastases (4-8). The gelatinase family is a subgroup of MMPs consisting of gelatinase A (MMP-2) and gelatinase B (MMP-9) (9). Gelatinase expression in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages, is highly regulated. Elevated levels of gelatinases have been found in tumors that are associated with a poor prognosis for cancer patients (10). A number of synthetic MMP inhibitors have been developed to block the activated MMPs in pathological conditions (11). A tumor cell targeting peptide, Gly-Ala-Cys-Leu-Arg-Ser-Gly-Arg-Gly-Cys-Gly (TCTP-1), was identified via phage display screening against MMP-9. Ujula et al. (12) prepared a cyc-cys cyclicpeptide, Gly-Ala-Cys-Leu-Arg-Ser-Gly-Arg-Gly-Cys-Gly-(PEG)_3_-DOTA-^68^Ga (^68^Ga-DOTA-TCTP-1), for preliminary evaluation of MMP-9 overexpression in tumors.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=MMP+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (MMP-9 (http://www.ncbi.nlm.nih.gov/gene/4318))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MMP-9 (http://www.ncbi.nlm.nih.gov/omim/120361))
- Clinical trials (MMP-9 (http://www.clinicaltrials.gov/ct2/results?term=MMP-9))
- Drug information in FDA (MMP-9 (http://google2.fda.gov/search?q=mmp-9&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=11))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TCTP-1+synthesis)]

A solution of 185 MBq (5 mCi) ^68^Ga and DOTA-TCTP-1 (30 nmol) was incubated in acetate buffer (pH 3.0) for 25 min at 95°C (12). ^68^Ga-DOTA-TCTP-1 was identified with high-performance liquid chromatography. ^68^Ga-DOTA-TCTP-1 exhibited a radiochemical purity of >95% and a specific activity of 2 GBq/µmol (54 mCi/µmol). ^68^Ga-DOTA-lactam-TCTP-1 and linear ^68^Ga-DOTA-lin-TCTP-1 (control linear peptide) were also prepared similarly with similar specific activity. ^68^Ga-DOTA-TCTP-1 has a log D_7.4_ value of -3.6.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TCTP-1+and+in+vitro)]

^68^Ga-DOTA-TCTP-1and the other two ^68^Ga-labeled peptides were stable in saline at room temperature for > 4 h (12). ^68^Ga-DOTA-TCTP-1 and ^68^Ga-DOTA-lin-TCTP-1 had half-lives of 2.5 h and 1 h in human plasma, respectively. ^68^Ga-DOTA-lactam-TCTP-1 was stable in human plasma up to 4 h.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TCTP-1+rodentia)]

Ujula et al. (12) performed ex vivo biodistribution studies of 19 MBq (0.51 mCi) ^68^Ga-DOTA-TCTP-1 in athymic rats (n = 3) bearing MMP-9 expressing C8161T/M1 human melanoma cell line at week 3 after the tumor inoculation. The tumor accumulation was 0.20 ± 0.03% injected dose/gram (ID/g) at 60 min after injection. The accumulations in the lung, liver, blood and muscle were 0.6 ± 0.2% ID/g, 0.4 ± 0.1% ID/g, 0.20 ± 0.03% ID/g, and 0.04 ± 0.01% ID/g, respectively. The tumor/muscle ratio was 4.8 ± 0.4. Approximately 71% and 35% of radioactivity in the plasma was intact ^68^Ga-DOTA-TCTP-1 at 15 min and 120 min after injection, respectively. As a comparison, ^68^Ga-DOTA-lactam-TCTP-1 and ^68^Ga-DOTA-lin-TCTP-1 exhibited tumor/muscle ratio of ~3.0. Immunohistochemistry of tumor sections showed the localization of MMP-9 in the endothelium and ECM of the blood vessels. However, there was only a weak correlation between MMP-9 levels and the ex vivo tumor accumulation. No blocking experiment was performed.

Positron emission tomography imaging showed that tumors were clearly visualized by ^68^Ga-DOTA-lactam-TCTP-1 and ^68^Ga-DOTA-TCTP-1 but not by ^68^Ga-DOTA-lin-TCTP-1 at 10-55 min after injection. The heart, liver, kidneys, and urinary bladder were also visualized. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TCTP-1+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TCTP-1+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=TCTP-1+human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Beaudeux J.L., Giral P., Bruckert E., Foglietti M.J., Chapman M.J. (2004). Matrix metalloproteinases, inflammation and atherosclerosis: therapeutic perspectives. Clin Chem Lab Med.
9 Nelson A.R., Fingleton B., Rothenberg M.L., Matrisian L.M. (2000). Matrix metalloproteinases: biologic activity and clinical implications. J Clin Oncol.
10 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
11 Skiles J.W., Gonnella N.C., Jeng A.Y. (2004). The design, structure, and clinical update of small molecular weight matrix metalloproteinase inhibitors. Curr Med Chem.
12 Ujula T., Huttunen M., Luoto P., Perakyla H., Simpura I., Wilson I., Bergman M., Roivainen A. (2010). Matrix metalloproteinase 9 targeting peptides: syntheses, 68Ga-labeling, and preliminary evaluation in a rat melanoma xenograft model. Bioconjug Chem.